# NIR2-Folate

Chemical name: | NIR2-Folate
Abbreviated name:
Synonym: | NIR2-Folic acid
Agent category: | Folic acid
Target: | Folate receptor
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | NIR2
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NIR2%20folate)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350-700 nm) are used. Near-infrared (NIR) fluorescence (700-1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals.

Folic acid is a water-soluble B vitamin (4) that is essential for methylation and DNA synthesis. The primary pathway for entry of folate into cells is through the facilitated transporter, which has a low affinity for folate (Michaelis constant (K_m_) = 1-5 μM). Some cells in the choroid plexus, kidney, lung, thyroid, spleen, placenta, and thymus also possess a higher affinity (dissociation constant (K_d_) = 0.5 nM) receptor that allows folate uptake via receptor-mediated endocytosis. Some human epithelial tumor cells were found to overexpress folate-binding protein (5). More than 90% of human ovarian and endometrial cancers express the high-affinity receptor, which is absent in normal tissues. Breast, colorectal, renal, and lung carcinomas also overexpress the folate receptor but at lower frequencies (20-50%). Activated macrophages, but not resting macrophages, have been also found to have folate receptor (6). Several folate-based conjugates (^111^In-DTPA-folate and ^99m^Tc-EC-folate) have been studied in tumor imaging.

Lin et al. (7) reported the synthesis of four new, water-soluble NIR cyanine fluorophores that have superior chemical stability and optical properties. One of the NIR dyes (NIR2) was conjugated to amino-derivatized folic acid to form NIR2-folate, which has an excitation maximum at 665 nm and an emission maximum at 686 nm. NIR2-folate is being developed as an optical imaging agent for detection of folate receptors in vivo.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=folate+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (folate receptor (http://www.ncbi.nlm.nih.gov/gene/2348))
- Articles in OMIM (folate receptor (http://www.ncbi.nlm.nih.gov/omim/136430))
- Clinical trials (folate receptors (http://www.clinicaltrials.gov/ct2/results?term=folate+receptor))
- Drug information in FDA (http://google2.fda.gov/search?q=folate+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NIR2%20folate%20and%20synthesis)]

Tung et al. (8) first reacted folic acid with a hydrophilic spacer, 2,2-(ethylenedioxy)-bis(ethylamine) (EDBEA) in anhydrous dimethyl sulfoxide with diisopropylcarbodiimide/N-hydroxysuccinimide (NHS) as the coupling agent. This converted the carboxyl group of folic acid into a functional amino group. The folate-EDBEA conjugate was purified by high-performance liquid chromatography (HPLC). The NHS ester of NIR2 was then coupled to the folate-EDBEA in 0.1 M NaHCO_3_/dimethylformamide. The final product, NIR2-folate, was purified by HPLC and was confirmed by mass spectroscopic analysis ([M]^+^: calculated, 1,401; found, 1,402). The absorption and fluorescence spectra of NIR2-folate showed the characteristics of both folic acid and NIR2.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NIR2%20folate%20and%20in%20vitro)]

The human nasopharyngeal carcinoma cell line KB (12 pmol/10^6^ cells) and ovarian cancer cell line OVCAR3 (1.4 pmol/10^6^ cells) have putative folate receptors, whereas cells from the human lung carcinoma A549 and fibrosarcoma HT1080 have no detectable folate receptors as determined by [^3^H]folate binding and internalization in cultures (8, 9). Cellular uptake of 50 nM folate by KB and OVCAR3 cells was saturable within 10-20 min of incubation and was completely blocked by excess folate or NIR2-folate. A549 and HT1080 cells (folate-receptor negative) did not show any specific uptake of folate. Fluorescence microscopy experiments to determine cellular distribution of NIR2-folate revealed bright signals only in the KB and OVCAR3 cells but not in the A549 and HT1080 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NIR2%20folate%20and%20rodentia)]

Tung et al. (8) performed a preliminary tumor imaging study of NIR2-folate in nude mice (n = 3) bearing an OVCAR3 xenograft model. Whole-body small-animal planar fluorescence reflectance imaging performed after injection of NIR2-folate (2 nmol/mouse) revealed intense tumor signals as early as 1 h after injection that reached a plateau at 24 h. No tumor signals were obtained with NIR2 alone at 1 or 24 h. Moon et al. (9) performed more extensive studies in KB and HT1080 tumors transplanted in nude mice (n = 36). The folate-receptor-positive KB tumors (870 ± 93 absorbance units (AU)) showed a 2.4-fold (P < 0.01) higher signal than the receptor-negative HT1080 tumors (366 ± 41 AU) at 24 h after NIR2-folate injection. Tumor/background ratios remained elevated for at least 24-48 h with a peak at 4 h. Tumor signals returned to background (115 ± 17 AU) at 120 h. Injection of NIR2 alone did not produce tumor signals above background. Injection of a mixture of NIR2-folate (2 nmol/mouse) and folate (600 nmol/mouse) reduced the tumor signals to background at 24 h.

Chen et al. (10) tested NIR2-folate for in vivo optical imaging of arthritis, using a lipopolysaccharide (LPS) intra-articular injection model. The intensities of the fluorescence signals for NIR2-folate (n = 12) and free NIR2 (n = 5) were compared between LPS-treated and control joints. The intensity of the fluorescence signal for NIR2-folate in inflammatory joints was significantly higher than in the normal control joints (2.3-fold; P < 0.001) at 24 h after intravenous (i.v.) NIR2-folate injection (2 nmol/mouse). The group receiving an i.v. injection of NIR2-free dye showed a persistently lower enhancement ratio (1.6-fold) than the group receiving an NIR2-folate injection (2 nmol/mouse). Folate pretreatment (1,200 nmol/mouse 5 min before injection of NIR2-folate) significantly lowered (P < 0.05) NIR2-folate accumulation in the inflamed joint, suggesting that the binding is specific to folate receptors. Fluorescence microscopy, histology, and immunohistochemistry validated the optical imaging results and indicated that activated macrophages were the primary source of NIR2-folate signals. Chen et al. (11) also reported detection of NIR2-folate signals from macrophages in dysplastic intestinal adenomas of APC^Δ468^-knockout mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NIR2%20folate%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NIR2%20folate%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NIR2%20folate%20and%20human)]

No publication is currently available.

## NIH Support

N01 C017014, P01 A154904, P50 CA86355, R24 CA92782, R33 CA88365

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Stanger O. (2002). Physiology of folic acid in health and disease. Curr Drug Metab.
5 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
6 Nakashima-Matsushita N., Homma T., Yu S., Matsuda T., Sunahara N., Nakamura T., Tsukano M., Ratnam M., Matsuyama T. (1999). Selective expression of folate receptor beta and its possible role in methotrexate transport in synovial macrophages from patients with rheumatoid arthritis. Arthritis Rheum.
7 Molina P.E. (2006). Opioids and opiates: analgesia with cardiovascular, haemodynamic and immune implications in critical illness. J Intern Med.
8 Tung C.H., Lin Y., Moon W.K., Weissleder R. (2002). A receptor-targeted near-infrared fluorescence probe for in vivo tumor imaging. Chembiochem.
9 Moon W.K., Lin Y., O'Loughlin T., Tang Y., Kim D.E., Weissleder R., Tung C.H. (2003). Enhanced tumor detection using a folate receptor-targeted near-infrared fluorochrome conjugate. Bioconjug Chem.
10 Chen W.T., Mahmood U., Weissleder R., Tung C.H. (2005). Arthritis imaging using a near-infrared fluorescence folate-targeted probe. Arthritis Res Ther.
11 Chen W.T., Khazaie K., Zhang G., Weissleder R., Tung C.H. (2005). Detection of dysplastic intestinal adenomas using a fluorescent folate imaging probe. Mol Imaging.